# Epidermal growth factor conjugated to near-infrared fluorescent quantum dots

Chemical name: | Epidermal growth factor conjugated to near-infrared fluorescent quantum dots
Abbreviated name: | EGF-QD
Synonym:
Agent Category: | Receptor ligand
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Near-infrared fluorescence (NIR fluorescence)
Source of signal / contrast: | Quantum dots (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Structure of EGF quantum dot as shown by Diagaradjane et. al. (1)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGF+quantum+dots)]

The epidermal growth factor (EGF) receptor (EGFR) is a membrane-spanning glycoprotein that mediates its activity through an intracellular tyrosine kinase (TK) signaling pathway and is considered to have a major role in the survival, growth, and proliferation of the mammalian cell (2). A mutated EGFR or its overexpression are thought to cause oncogenic transformation of cells that culminates in the development and progression of various types of cancers (2, 3). Because of its involvement in the cancer process, the EGFR and its associated TKs are targets of a variety of small-molecule and monoclonal antibody (MAb) inhibitors for the management and treatment of cancers (2, 3). However, these inhibitors are not entirely effective because patients either develop resistance to the small-molecule drugs or exhibit little to no response to the MAb treatment (4, 5). Several drugs and MAbs (and combinations of the two) are approved by the United States Food and Drug Administration for evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR+inhibitors) for the treatment of cancers. Some investigators in the field of anticancer drug development believe non-invasive imaging techniques used to visualize EGFR overexpression in tumors versus surrounding tissues could possibly predict the effectiveness of a therapeutic regimen directed against this ailment (1, 2, 6, 7). Although highly targeted radiolabeled MAb probes (~150 kDa) have been developed for the imaging of EGFR expression, these agents are not very useful because they have a large size and may not penetrate deeply into all tumors. Moreover, these molecules have long blood circulation half-lives, and the radiolabels tend to accumulate in organs involved in excretion of the radioactivity, thereby masking the metastatised tumors in these organs during imaging (8). The use of radiolabeled antibody fragments (~25 kDa) for EGFR imaging has also been attempted, but at present these agents appear to be primarily in preclinical development (9, 10).

As an alternative to radiolabeled probes, some investigators developed fluorescent dyes, which are easy and inexpensive to synthesize and do not expose a patient to radiation, and linked them to either anti-EGFR Abs or their fragments for the in vivo imaging of EGFR in animals (11, 12). However, these dyes show characteristic photobleaching, so the images must be acquired quickly; this is an imaging limitation because the fluorescence may not last for sufficiently prolonged periods. Therefore, it was necessary to develop an optical imaging agent with photo-stable characteristics to obtain high-quality images (1). Subsequently, fluorescent semiconductor quantum dots (QDs) were developed for molecular imaging and were shown to have superior imaging characteristics compared with the fluorescent dyes. The QDs have an emission spectra (20–30 nm) over a large excitation spectral range, have a longer fluorescence half-life (5–40 ns) compared with the dyes (0.5–2.0 ns), are resistant to photobleaching, and can be conjugated to a variety of biomolecules including peptides, nucleotides, etc (1, 7, 13, 14). Diagaradjane et al. conjugated EGF to near-infrared fluorescent QDs (EGF-QDs) and used them to image EGFR expression in human colon cancer cell lines under in vitro conditions and in xenograft tumors in mice (1). From these studies the investigators concluded that the EGF-QDs were a suitable imaging agent to determine the level of EGFR expression in cell lines and xenograft tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=egf+quantum+dot+synthesis)]

The synthesis of EGF-QDs was described by Diagaradjane et al. (1). Human recombinant EGF was obtained from commercial sources, and the QDs (emission maximum at 800 nm) were activated as detailed elsewhere (1). The activated QDs were purified on a Sephadex G-25 PD-10 desalting column with phosphate-buffered saline (PBS; pH 7.4) as the elution buffer. In a separate reaction, EGF was reduced with dithiothreitol for 30 min to obtain a product containing free sulfhydryl groups. The reduced EGF (r-EGF) was purified as described above for the activated QDs. The activated QDs and the r-EGF were mixed and allowed to conjugate for 1 h at room temperature. The reaction was quenched with β-mercaptoethanol, and the product was concentrated on a spin column (cut-off limit of spin column not provided). Purification of the EGF-QDs was performed with gel-filtration on a PD-10 column containing Sephadex G-200 with PBS (pH 7.4) as the elution buffer. The estimated concentrations of EGF and the QDs in the final product were determined to be 2.9 and 0.75 μmol/L, respectively, indicating there were four molecules of EGF conjugated to each QD (1). The storage conditions and stability of the EGF-QDs were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=egf+quantum+dots+in+vitro)]

With the use of an enzyme-linked immunosorbant assay, the native and r-EGF were reported to have a similar affinity for an anti-EGF Ab (1). However, Western blot analysis showed that, compared with the native EGF, the r-EGF induced a minimal phosphorylation of the EGFR under in vitro conditions. From these results the investigators assumed that the EGF-QDs would probably bind the EGFR on the cell surface, but would not trigger the EGFR signaling pathway in the cell, and the conjugated QDs would serve as good imaging probes.

Specificity of the EGF-QDs was determined by exposing human colorectal cancer HCT116 cells, which have a moderate expression of EGFR, and DiFi, which have high EGFR expression, to the conjugated QDs (1). Chinese hamster ovarian cancer K1 cells (CHO K1) that do not express the EGFR were used as controls for the study. Background fluorescence from the different cells was measured with confocal microscopy before the cells were exposed to the EGF-QD conjugate for 20 min at 37°C. Two controls were set up for this study. As the first control, the different cell lines were respectively exposed to the native QDs alone. The second control involved pretreatment of the various cell lines with cetuximab, an anti-EGFR monoclonal antibody, for 45 min at 37°C followed by exposure to the EGF-QD nanoprobe. Fluorescent confocal microscopy showed that only the HCT116 and DiFi cells exposed to the EGF-QDs exhibited fluorescence within 5 min of treatment with the probe, and the signal correlated with the EGFR expression levels of these cells. No fluorescent signal was generated by the HCT116 and DiFi cells that were exposed to EGF-QDs after the cetuximab pretreatment or when exposed to the native QDs alone. From these studies the investigators concluded that the EGF-QDs bound specifically to the EGFR on these cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=egf+quantum+dots+rodentia)]

In vivo imaging studies were performed with immunocompromised male nude mice bearing HCT116 xenograft tumors on the right flank (1). When the tumor size reached 0.8–1 cm in diameter, the animals were administered intravenously with either QDs alone (n = 7 animals) or the EGF-QD nanoprobe (n = 8 animals) through the tail vein. Near-infrared fluorescence imaging was performed on the animals at various time points starting at 3 min after treatment for up to 24 h. Among the various organs, the liver and the spleen showed the highest fluorescence with the QDs and with the EGF-QDs at 3 min after injection. This fluorescence decreased rapidly by 1 h after the injection, and only the EGF-QDs gave a high signal in these organs at 4 h post-injection (p.i.). By 24 h the QD and EGF-QD fluorescence reached baseline levels.

Using fluorescence obtained from the two groups of animals, the tumor/background ratios for the mice injected with the QDs or the EGF-QDs were determined at various time points (1). The QDs and the EGF-QDs showed a rapid influx at 3 min p.i. that gradually cleared by 60 min. The investigators reported that during this time the animals injected with EGF-QD exhibited a ~50% higher fluorescence compared with animals injected with the QDs alone. The clearance rate constants for the QDs and the EGF-QDs were 1.26 ± 0.38 per h and 0.57 ± 0.12 per h, respectively, during this period, and the half-lives of the QDs and the EGF-QDs were estimated to be 0.64 ± 0.15 h and 1.40 ± 0.32 h, respectively. By 24 h p.i. the fluorescence was reduced to background levels for both the QD and EGF-QD nanoprobes. The 4 h p.i. time point was reported to be the discriminating time point for the EGF-QD and QD fluorescence with the tumor/background ratios being 1.93 ± 0.27 and 0.86 ± 0.10, respectively (P < 0.03).

Pretreatment of the animals with cetuximab before the EGF-QD treatment abolished the tumor fluorescence observed in the mice that were not pretreated (1). From this result the investigators concluded that the EGF-QDs had favorable pharmacokinetics and specificity for the EGFR under in vivo conditions.

For ex vivo microscopic fluorescence imaging, the various organs were extracted at 4 and 24 h p.i. from animals injected with either the QDs or the EGF-QDs (1). The liver and spleen showed the highest fluorescence with both probes at the two time points. The lungs had a higher intensity of fluorescence at 4 h than at 24 h. The kidneys had a higher fluorescence at 24 h than at 4 h with both probes. This was attributed to the possibly delayed renal clearance of the fluorescent probes from the animals.

A semiquantitative analysis of average fluorescence emitted from tissue homogenates was also performed at 4 and 24 h p.i (1). A significantly higher average fluorescence was reported in tissues from animals treated with EGF-QDs (P = 0.0008) compared with tissues obtained from the QD-treated animals. At 24 h p.i. no significant difference in average fluorescence (P = 0.4137) from the tissue homogenates of both animals groups was reported.

With results obtained from the various studies, the investigators concluded that the EGF-QDs had suitable pharmacokinetic, affinity, and specificity properties for use as an imaging tool to determine EGFR expression levels in xenograft tumors in mice (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGF+quantum+dots+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGF+quantum+dots+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGF+quantum+dots+Human+Studies)]

No references are currently available.

## References

1 Diagaradjane P., Orenstein-Cardona J.M., Colon-Casasnovas N.E., Deorukhkar A., Shentu S., Kuno N., Schwartz D.L., Gelovani J.G., Krishnan S. (2008). Imaging epidermal growth factor receptor expression in vivo: pharmacokinetic and biodistribution characterization of a bioconjugated quantum dot nanoprobe. Clin Cancer Res.
2 Mishani E., Abourbeh G., Eiblmaier M., Anderson C.J. (2008). Imaging of EGFR and EGFR tyrosine kinase overexpression in tumors by nuclear medicine modalities. Curr Pharm Des.
3 Hosokawa, S., S. Toyooka, Y. Fujiwara, M. Tokumo, J. Soh, N. Takigawa, K. Hotta, T. Yoshino, H. Date, M. Tanimoto, and K. Kiura, Comprehensive analysis of EGFR signaling pathways in Japanese patients with non-small cell lung cancer. Lung Cancer, 2009
4 Kancha R.K., von Bubnoff N., Peschel C., Duyster J. (2009). Functional analysis of epidermal growth factor receptor (EGFR) mutations and potential implications for EGFR targeted therapy. Clin Cancer Res.
5 Patel D.K. (2008). Clinical use of anti-epidermal growth factor receptor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
6 Gleysteen J.P., Newman J.R., Chhieng D., Frost A., Zinn K.R., Rosenthal E.L. (2008). Fluorescent labeled anti-EGFR antibody for identification of regional and distant metastasis in a preclinical xenograft model. Head Neck.
7 Yang L., Mao H., Wang Y.A., Cao Z., Peng X., Wang X., Duan H., Ni C., Yuan Q., Adams G., Smith M.Q., Wood W.C., Gao X., Nie S. (2009). Single chain epidermal growth factor receptor antibody conjugated nanoparticles for in vivo tumor targeting and imaging. Small.
8 Pantaleo, M.A., M. Nannini, A. Maleddu, S. Fanti, C. Nanni, S. Boschi, F. Lodi, G. Nicoletti, L. Landuzzi, P.L. Lollini, and G. Biasco, Experimental results and related clinical implications of PET detection of epidermal growth factor receptor (EGFr) in cancer. Ann Oncol, 2008
9 Huang L., Gainkam L.O., Caveliers V., Vanhove C., Keyaerts M., De Baetselier P., Bossuyt A., Revets H., Lahoutte T. (2008). SPECT imaging with 99mTc-labeled EGFR-specific nanobody for in vivo monitoring of EGFR expression. Mol Imaging Biol.
10 Gainkam L.O., Huang L., Caveliers V., Keyaerts M., Hernot S., Vaneycken I., Vanhove C., Revets H., De Baetselier P., Lahoutte T. (2008). Comparison of the biodistribution and tumor targeting of two 99mTc-labeled anti-EGFR nanobodies in mice, using pinhole SPECT/micro-CT. J Nucl Med.
11 Barrett T., Koyama Y., Hama Y., Ravizzini G., Shin I.S., Jang B.S., Paik C.H., Urano Y., Choyke P.L., Kobayashi H. (2007). In vivo diagnosis of epidermal growth factor receptor expression using molecular imaging with a cocktail of optically labeled monoclonal antibodies. Clin Cancer Res.
12 Koyama Y., Barrett T., Hama Y., Ravizzini G., Choyke P.L., Kobayashi H. (2007). In vivo molecular imaging to diagnose and subtype tumors through receptor-targeted optically labeled monoclonal antibodies. Neoplasia.
13 Derfus A.M., Chen A.A., Min D.H., Ruoslahti E., Bhatia S.N. (2007). Targeted quantum dot conjugates for siRNA delivery. Bioconjug Chem.
14 He H., Xie C., Ren J. (2008). Nonbleaching fluorescence of gold nanoparticles and its applications in cancer cell imaging. Anal Chem.